# N-(2,3-Dihydroxypropyl)-N´-(2-hydroxyethyl)-5-[N-(2,3-dihydroxypropyl)acetamido]-2,4,6-triiodoisophthalamide

Chemical name: | N-(2,3-dihydroxypropyl)-N´-(2-hydroxyethyl)-5-[N-(2,3-dihydroxypropyl)acetamido]-2,4,6-triiodoisophthalamide
Abbreviated name: | Ioxilan
Synonym: | Oxilan^®^, 5-(N-2,3-dihydroxypropylacetamido)-2,4,6-triiodo-N-(2-hydroxyethyl)-N´-(2,3-dihydroxypropyl)-isophthalamide, ioxitol
Agent Category: | Compound
Target: | None
Target Category: | Nontargeted filling of blood vessels and tissues
Method of detection: | X-ray, CT
Source of signal: | Iodine
Activation: | No
Studies: | - In vitro; - Rodents; - Other non-primate mammals; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Ioxilan%20OR%20Oxilan)]

N-(2,3-dihydroxypropyl)-N´-(2-hydroxyethyl)-5-[N-(2,3-dihydroxypropyl)acetamido]-2,4,6-triiodoisophthalamide (ioxilan) is a nonionic X-ray contrast agent approved by the United States Food and Drug Administration for X-ray imaging contrast enhancement (1, 2). Ioxilan can be administered intravenously for excretory urography and contrast-enhanced computed tomography (CT) imaging of the head and body (3). Ioxilan can also be given intraarterially for cerebral arteriograpy, coronary arteriography and left ventriculography, visceral angiography, aortography, and peripheral arteriography.

Techniques for X-ray imaging (planar and tomographic) depend on tissue density differences that provide the image contrast produced by X-ray attenuation between the area of interest and its surrounding tissues (4, 5). Contrast enhancement (opacification) with use of contrast agents increases the degree of contrast and improves the differentiation of pathologic processes from normal tissues. Because iodine, an element of high atomic density, causes high attenuation of X-rays within the diagnostic energy spectrum, water-soluble and reasonably safe iodinated contrast agents in intravenously injectable forms have been developed for clinical applications (6, 7).

Water-soluble, intravenous X-ray contrast agents are generally organic iodine compounds that contain one or more tri-iodinated benzene rings (8, 9). When injected intravenously, they are largely distributed in the extracellular fluid space and excreted unchanged by the kidneys (10). Contrast enhancement of a region of interest depends on the route of administration, delivery of the agent to the area by blood flow, and the final iodine concentration in the region. There are two basic types of these compounds: ionic and nonionic agents. The first monomeric ionic compound, in the form of 2,4,6-triiodobenzene acetrizoic acid, was synthesized by Wallingford (6). Most ionic contrast agents are derived from the basic structures of 3,5-diamino-2,4,6-triiodobenzoic acid, 5-amino-2,4,5-triiodoisophthalic acid, or 2,4,6-triiodobenzene-1,3,5-tricarbonic acid. In addition to monoacidic ionic dimers, nonionic compounds have also been developed to improve the tolerance of these agents in patients. The basic strategy of developing nonionic agents is to eliminate the electrical charges in the structure, which will lead to a reduction in osmolality of the compound. Because osmolality is related to the number of particles in solution, the challenge is to reduce the number of particles but maintain the iodine concentration (11). This is generally achieved by conversion of the carboxyl groups to hydroxyalkylamide groups (12).

As a low-osmolar nonionic monomer, ioxilan was developed in an effort to increase the safety and tolerance of X-ray contrast agents. The development of ioxilan was based on the belief that the introduction of a double methylene as a hydrophobic region and masking it with a hydrophilic hydroxyl group could lower the osmolality without adversely affecting the biological tolerance (13). Ioxilan is available commercially in preparations of 300 mg I/ml (632 mg ioxilan) and 350 mg I/ml (727 mg ioxilan). Their measured osmolality values (mOsm/kg water) at 37ºC are 585 and 695, respectively. The viscosity values (cP) at 37ºC are 5.1 and 8.1, respectively.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Ioxilan%20OR%20Oxilan%29%20AND%20synthesis)]

Ioxilan can be synthesized in a variety of ways (13). Sovak and Ranganathan (14, 15) reported the eight-step conversion of ioxithalamic acid into ioxilan. Briefly, ioxithalamic acid was alkylated and acetylated into 5-(N-2,3-diacetoxypropylacetamido)-2,4,6-triiodo-N-(2-acetoxyethyl)-isophthalamic acid. The yield was 97%. This was reacted with thionyl chloride and heated at 60-65ºC for 1 h to form an acyl-chloride with a yield of 96%. The N-alkylated, acetylated, ioxithalamic acid chloride was amidated with trans-dioxepane and then deprotected to produce an aminothreitol derivative. The resulting product was further amidated with 1-amino-2,3-propanediol in triethylamine at room temperature for 8 h with a 87.9% yield. The amidated compound was then deacetylated in methanol at pH 13 for 30 min to yield (80%) the final product of ioxilan.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Ioxilan%20OR%20Oxilan%29%20AND%20%28%22in%20vitro%22%29)]

Violon studied the in vitro osmolality of ioxilan and seven other monomeric nonionic agents (16). The author concluded that both the hydrophilic and hydrophobic characteristics of a molecule are important in the determination of the osmolality. Parvez and Patel (17) studied the in vitro effect of ioxilan on human erythrocytes. Ioxilan (7, 14, and 35 mg I/ml) was incubated with freely drawn and ethylenediaminetetraacetic acid-anticoagulated human blood, heparinized whole human blood, or platelet-rich plasma at 37ºC for 60 min, 30 min, or 3 min, respectively. No change was observed in the red cell morphology study. Ioxilan inhibited adenosine diphosphate−induced platelet aggregation in a manner similar as iopamidol. It did not activate the serum complement system.

Rabbit thoracic aortas (aortic rings) were used to study the functional and morphologic effects of ioxilan on endothelial cells in vitro (18). The ability of the endothelial cells to release an endothelium-derived relaxing factor was tested by measuring the dilator response to acetylcholine. After incubation with ioxilan (350 mg I/ml), the percentages (%) of retained dilator activity to acetylcholine (0.2 μmol/L) were 95.1 ± 15.2 and 114.5 ± 29.8 (n = 3) for incubation times of 15 min and 60 min, respectively. In comparison, sodium meglumine diatrizoate (370 mg I/ml0, a high-osmolar ionic contrast agent, had values of 48.6 ± 6.9% and 0 ± 0%, respectively. Scanning and transmission electron micrographs showed that ioxilan produced irregularities in the cell borders and in some vesicles. Similar effects were produced by another nonionic monomer, iohexol (350 mg I/ml). Schneider and Rand (19) showed that ioxilan, iohexol, and diatrizoate all caused a direct chemotoxic effect on smooth muscle cells in isolated rabbit aortas. The study suggested that the effects were caused by activating the production of a cyclic nucleotide.

Lasser and Lyon (20) studied the in vitro inhibition of angiotensin-converting enzyme (ACE) by ioxilan. In a pattern similar to six other commercial ionic and nonionic contrast agents, ioxilan (30% iodine) showed an inhibitory effect on ACE under the studied condition.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Ioxilan%20OR%20Oxilan%29%20AND%20rodentia)]

Thomsen et al. (21, 22) studied the effects of ioxilan on urine profiles in rats. Ioxilan (350 mg I/kg) was given by i.v. administration. Ioxilan caused albuminuria, higher excretion of both glucose and L-γ-glutamyltransferase, and tubular dysfunction. Similar effects were observed with iohexol. In comparison, diatrizoate caused significantly greater effects on the kidneys. These renal effects were confirmed in a rat model of nephropathy induced by intramuscularly administered glycerol (23). Ioxilan did not appear to aggravate Fanconi’s syndrome (tubulointerstitial nephropathies) in rats induced by i.v. injection of sodium maleate in rats (24).

Harnish et al. (25) investigated the effects of ioxilan on the blood-brain barrier (BBB) in hypertensive rats. Ioxilan in doses of 350 mg I/ml and 175 mg I/ml were injected into the carotid artery. No significant BBB damage assessed by ^14^C-labeled inulin was found in normal and hypertensive rats with elevated blood pressure of 165-190 mm Hg.

Sovak et al. (2) used a psychopharmacological method, conditioned taste aversion (CTA), to quantify the vascular pain caused by ioxilan in rats. The percentage of CTA to ioxilan was -9.99 ± 22.31 (n = 15). In comparison, iohexol and iopamidol had values of -56.33 ± 20.81 and -33.08 ± 24.37, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Ioxilan%20OR%20Oxilan%29%20AND%20%28dog%20OR%20pig%20OR%20rabbit%20OR%20sheep%29)]

The effects of ioxilan on renal size, renal profiles and blood profiles were studied in rabbits (26). Ioxilan (350 mg I/ml; 5 ml/kg) did not cause significant changes in any of the studied profile components. Moore et al. (27) reported that ioxilan (300 mg I/ml) produced no pathologic response in the rabbit fallopian tube or peritoneal cavity. Thurmond et al. (28) showed that ioxilan (350 mg I/ml) administration by direct intratubular injection caused 0.9 (average inflammation number) fallopian tube inflammation in 10 rabbits 24 h after injection. The average inflammation numbers were 0 (n = 3) and 0.7 (n = 5) for 4 days and 2 weeks, respectively. In comparison, the average inflammation numbers for diatrizoate (52%) were 1.4 (n = 5), 0 (n = 3), and 0.7 (n = 3), respectively. The authors suggested that ioxilan could be clinically acceptable for direct injection into the human fallopian tube.

Eisenberg et al. (29) evaluated the early and delayed inflammatory response of the peritoneal surfaces to ioxilan in guinea pigs. Animals given intraperitoneally injections of ioxilan (300 mg I/ml) showed only two inflammatory responses (n = 5) at 7 days and no inflammation at 1 day or 30 days after injections. In comparison, diatrizoate sodium (300 mg I/ml) showed two, three, and one inflammatory responses at 1, 7, and 30 days, respectively.

In a dog study (n = 6), Katzberg et al. (1) demonstrated that i.v. ioxilan administration (350 mg I/ml; 2 m/kg) produced satisfactory nephrograms and pyelograms. The effects of ioxilan on systemic and renal hemodynamics were minimal and similar to those of iohexol (350 mg I/ml). Izci et al. (30) reported that no adverse clinical signs were observed in dogs (n = 6) that received i.v. ioxilan (350 mg I/ml or 700 mg I/kg). Blood samples were collected to evaluate acid-base, venous blood gas status (pH, PCO_2_, PO_2_, HCO_3_−, BE, O_2_) and electrolytes (Na^+^, Ca^++^, K^+^). No long-lasting or major effects of any of these studied parameters were found. Nakamura et al. (31) found that ioxilan radiographic images (cerebral angiography, aortofemoral angiography, and left ventriculography) and cardiovascular changes in dogs (n = 4-5) after administration of ioxilan (350 mg I/ml) were similar to radiographic images after administration of iohexol (350 mg I/ml) and iopamidol (370 mg I/ml). In comparison, diatrizoate (76%) had a greater effect on studied cardiovascular parameters. Misumi et al. (32) reported that ioxilan (350 mg I/ml) had low incidence of ventricular fibrillation in dogs, and they suggested that this property might be attributable to its optimal sodium concentration of 9 mmol/L.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Ioxilan%20OR%20Oxilan%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Ioxilan%20OR%20Oxilan%29%20AND%20humans)]

Callantine et al. (33) conducted a phase I study of ioxilan (300 and 350 mg I/ml) at four dose levels (100, 300, 500, and 700 mg I/kg) in 24 human volunteers. After i.v. administration, there were no clinically significant changes in the physical examination findings (ophthalmic and neurologic evaluations), vital signs, or electrocardiograms. A mild and transient increase in blood pressure and heart rate was observed at 3 min after injection in some patients. No significant changes were found in serum chemistries, hematologic values, or renal functions. Pharmacokinetic data revealed no significant differences in plasma concentrations over time with either ioxilan concentrations. There was an initial rapid distribution phase (t_½α_ = 18.01 ± 3.12 min) which was followed by a slower elimination phase (t_½β_ = 107.43 ± 3.92 min). Ioxilan was excreted primarily by the kidneys with a volume of distribution of 19.5 L and renal clearance of 116.5 ml/min. About 93% of the dose was excreted unchanged in the urine within 24 h.

McIntosh and Reed (34) reported the results of a phase III clinical studies for ioxilan. There were 835 patients who received ioxilan (300 or 350 mg I/ml). The results were compared with those of iohexol in 523 patients. Overall clinical adverse events showed that 2 patients experienced a total of four adverse events. In comparison, the iohexol group had 3 patients who experienced five adverse events. The hepatic, hematologic, and renal safety profiles, as well as patient tolerance for pain and warmth of ioxilan were similar to those of iohexol. There was no evidence of in vitro or in vivo activation of blood coagulation. Images (aortofemoral and visceral arteriography, coronary and left ventricular angiography, cerebral arteriography, excretory urography, and body and head CT) were reviewed by two blinded independent readers reported that 97% of 358 ioxilan images were of diagnostic quality. In comparison, iohexol had 98% of 375 iohexol images were of diagnostic quality.

## References

1 Katzberg RW, Donahue LA, Morris TW, Ventura JA, Krutchen AE, Proskin HM, Sovak M, Cos LR. (1990). Ioxilan, a third generation low osmolality nonionic contrast medium. Systemic and renal hemodynamic effects. Invest Radiol.
2 Sovak M Halkovich CA Foster SJ Current contrast media and ioxilan. Comparative evaluation of vascular pain by aversion conditioning Invest Radiol 1988 23Suppl 1S84 S87 3198369
3 3. Oxilan (Ioxilan Injection) 300 mg/ml, Oxilan (Ioxilan Injection) 350mg/ml, Nonionic Contrast Agents, Package Insert. . 2002, Guerbet LLC. p. 1-2.
4 4. Swanson DP, Alpern MB. Contrast media for computed tomography: Intravascular, intracavitary, xenon, reticuloendothelial, in Pharmaceuticals in medical imaging, D.P. Swanson, H. M. Chilton and J. H. Thrall, Editor. 1990, Macmillan Publishing Company: . p. 99-124.
5 5. Hoey GB, Smith KR. Chemistry of X-ray contras media, in Radiocontrast agents, M. Sovak, Editor. 1984, Springer-Verlag: . p. 23-125.
6 Wallingford VH. (1953). The development of organic iodine compounds as x-ray contrast media. J Am Pharm Assoc Am Pharm Assoc Baltim.
7 Sovak M, Ranganathan R, Lang JH, Lasser EC. (1977). Concepts in design of improved intravascular contrast agents. European Society of cardiovascular Radiology, (May): p. 25-27.
8 8. Gries H. Chemistry of X-ray contrast agents, in Textbook of contrast media, P. Dawson, D.O. Cosgrove, and R.G. Grainger, Editors. 1999, Isis Medical Media Ltd.: . p. 15-22.
9 Almen T. (1969). Contrast agent design. Some aspects on the synthesis of water soluble contrast agents of low osmolality. J Theor Biol.
10 10. Dawson P. Pharmacokinetics of water-soluble iodinated X-ray contrast agents, in Textbook of contrast media, P. Dawson, D.O. Cosgrove, and R.G. Grainger, Editors. 1999, Isis Medical Media . p. 61-74.
11 Ralston WH Robbins MS Coveney J Blair M Acute and subacute toxicity studies of ioversol in experimental animals Invest Radiol 1989 24Suppl 1S2 S9 2592169
12 Almen T Development of nonionic contrast media Invest Radiol 1985 201 SupplS2 S9 2579043
13 Sovak M The need for improved contrast media. Ioxilan: updating design theory Invest Radiol 1988 23Suppl 1S79 S83 3058636
14 Sovak M, Ranganathan R. (1990). Non-ionic Polyol Contrast Media From Ionic Patent 4,954,348. , Cook Imaging Corporation: p. 8.other.
15 Sovak M, Ranganathan R. (1991). Non-ionic Contrast Media from Ionic Patent 5,035,877. , Cook Imaging Corporation: p. 7.other.
16 Violon D. (1997). Analysis of the factors influencing the osmolality of eight monomeric nonionic iodinated contrast medium molecules. Invest Radiol.
17 Parvez Z Patel NB Effect of a new nonionic contrast agent, ioxilan, on human erythrocytes and the hemostatic and serum complement pathways Invest Radiol 1988 23Suppl 1S182 S185 3198340
18 Schneider KM Ham KN Friedhuber A Rand MJ Functional and morphologic effects of ioxilan, iohexol, and diatrizoate on endothelial cells Invest Radiol 1988 23Suppl 1S147 S149 3264276
19 Schneider KM Rand MJ Vasodilatation and vasoconstriction in the rabbit isolated aorta. Effects of ioxilan, iohexol, and diatrizoate Invest Radiol 1988 23Suppl 1S150 S152 3198336
20 Lasser EC, Lyon SG. (1990). Inhibition of angiotensin-converting enzyme by contrast media. I. In vitro findings. Invest Radiol.
21 Thomsen HS, Dorph S, Mygind T, Sovak M, Nielsen H, Rygaard H, Larsen S, Skaarup P, Hemmingsen L, Holm J. (1988). Intravenous injection of ioxilan, iohexol and diatrizoate. Effects on urine profiles in the rat. Acta Radiol.
22 Thomsen HS Dorph S Mygind T Hemmingsen L Holm J Larsen S Nielsen H Rygaard H Skaarup P Urine profiles following intravenous diatrizoate, iohexol, or ioxilan in rats Invest Radiol 1988 23Suppl 1S168 S170 3198338
23 Thomsen HS, Larsen S, Hemmingsen L, Holm J, Skaarup P. (1989). Nephropathy induced by intramuscularly administered glycerol and contrast media in rats. A comparison between diatrizoate, iohexol and ioxilan. Acta Radiol.
24 Thomsen HS Dorph S Mygind T Nielsen H Rygaard H Larsen S Skaarup P Hemmingsen L Holm J Do contrast media aggravate Fanconi's syndrome in rats? A comparison of diatrizoate, iohexol, and ioxilan Invest Radiol 1988 23Suppl 1S164 S167 3198337
25 Harnish PP, Krutchen A, Mukherji M. (1989). Intravascular contrast media and the blood-brain barrier. Testing the new nonionic agent ioxilan. Invest Radiol.
26 Rygaard H, Dorph S, Thomsen HS, Mygind T, Nielsen H, Larsen S, Skaarup P, Hemmingsen L, Holm J. (1988). Effects of intravenous injection of diatrizoate, iohexol or ioxilan on renal size, urine profiles and blood profiles in the rabbit. Acta Radiol.
27 Moore DE, Segars JH, Winfield AC, Page DL, Eisenberg AD, Holburn GE. (1990). Effects of contrast agents on the fallopian tube in a rabbit model. Radiology.
28 Thurmond AS, Hedgpeth PL, Scanlan RM. (1991). Selective injection of contrast media: inflammatory effects on rabbit fallopian tubes. Radiology.
29 Eisenberg AD, Winfield AC, Page DL, Holburn GE, Schifter T, Segars JH. (1989). Peritoneal reaction resulting from iodinated contrast material: comparative study. Radiology.
30 Izci C, Ogurtan Z, Ceylan C. (2004). Effects of hyperosmolar ionic and low osmolar non-ionic contrast media on acid base, blood gas and electrolyte status in dogs. J Vet Med A Physiol Pathol Clin Med.
31 Nakamura H, Kurata M, Haruta K, Takeda K. (1994). Effects of ionic and nonionic contrast media on cardiohemodynamics and quality of radiographic image during canine angiography. J Vet Med Sci.
32 Misumi K, Tateno O, Fujiki M, Miura N, Sakamoto H. (2000). The risk of contrast media-induced ventricular fibrillation is low in canine coronary arteriography with ioxilan. J Vet Med Sci.
33 Callantine MR Sovak M Lu HP Ioxilan. Initial clinical observations Invest Radiol 1990 25Suppl 1S107 S108 2283219
34 McIntosh CL Reed R Ioxilan injection. An overview and results of aortofemoral arteriography study Invest Radiol 1994 29Suppl 2S40 S42 7928267